# ^111^In-Labeled MLS128 anti-Tn murine monoclonal antibody

Chemical name: | ^111^In-Labeled MLS128 anti-Tn murine monoclonal antibody
Abbreviated name: | ^111^In-MLS128
Synonym:
Agent Category: | Antibody
Target: | Tn antigen
Target Category: | Tumor-associated carbohydrate antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=%22Tn%20antigen%22)]

Tn antigen is a tumor-associated carbohydrate epitope (N-acetyl-galactosamine (GalNAc)-O-Ser/Thr (GalNAca-O-Ser/Thr)) (1-3). The ^111^In-labeled anti-Tn murine monoclonal antibody (^111^I-MLS128 mAb) was developed for in vivo imaging of Tn antigen-expressing tumors (4).

Altered glycosylation on the cell surface is a hallmark of malignant transformation and tumor progression. Incomplete synthesis of the carbohydrate chains and precursor accumulation result in loss of the normal carbohydrate antigens and high expression of the tumor-associated carbohydrate antigens (5-7). Lewis Y, TF, Globo H, GM2, polysialic acid, sialyl Lewis A, Tn, and sialyl Tn are some of the antigens investigated intensively as diagnostic markers or as vaccine antigens (6-9). Tn antigen was first reported as a tumor-associated antigen nearly 40 years ago (10). It is composed of a single GalNAc glycan residue attached via an α-linkage to either the serine (Ser) or the threonine (Thr) of a polypeptide chain (7, 9). In normal tissues, Tn antigen is generally masked by covalently bound terminal carbohydrate moieties, but in tumors it is unmasked because of defective O-glycosylation. Accordingly, Tn antigen is rarely expressed in normal tissues, but it is widely expressed in human carcinomas or hematological cancers. It has been reported that Tn antigen is expressed in 70–90% of breast, colon, lung, bladder, cervical, ovarian, stomach, and prostate tumors (1, 3, 5). The expression levels of the Tn antigen are closely associated with tumor aggressiveness and poor survival of patients (6, 8). In addition, Tn antigen is recognized by the human immune system as a novel epitope, provoking immune responses in patients. There is a strong correlation among the expression of the Tn antigen, the development of the spontaneous antibodies against Tn, and the prognosis of the patients with carcinomas. Clinical trials are under way to deliberately provoke or enhance human immune responses by injecting patients with synthetic peptide antigens bearing Tn structure (3, 6, 11-13).

Tn antigen has attracted significant interest as a target for tumor diagnosis and immunotherapy. A number of anti-Tn IgG and IgM antibodies have been generated and investigated for their imaging feasibilities and anti-tumor activities (2, 4, 14-20). The results are generally inconsistent. There are still some issues to be resolved, such as immunogenicity, reduced effectiveness in vivo, and cross-reactivity against type-A blood antigen. Yao et al. developed a ^111^In-labeled anti-Tn MLS128 mAb and tested its feasibility for in vivo imaging of Tn-expressing colorectal tumor xenografts (4).

Note: Investigators from the same research group as Yao et al. also labeled the anti-Tn MLS128 mAb directly with ^125^I/^131^I (^125^I/^131^I-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) and investigated its biodistribution and the feasibility of imaging tumors in mice bearing LS180 tumor xenografts. They also tested the imaging feasibilities of two-step targeting with biotinylated MLS128 (Bt-MLS128) and ^125^I-labeled streptavidin (^125^I-SA) (Bt-MLS128-^125^I-SA (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)), and three-step targeting with Bt-MLS128, SA, and ^111^In-biotin (Bt-MLS128-SA-^111^In-biotin (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) in mice with LS180 tumor xenografts (4, 15-18, 21).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

The anti-Tn MLS128 mAb is a mouse IgG3 antibody with κ light chain. It was produced by immunizing mice with LS180 human colorectal cancer cells (19), and the antibody was purified from the ascitic fluid of hybridoma-bearing mice with protein A affinity chromatography. The antibody was labeled with ^111^In using 1-(4-isothiocyanatobenzyl)ethylenediaminetetraacetic acid (SCN-Bz-EDTA) as a bifunctional chelating agent. Briefly, the antibody solution in 0.05 M borate-buffered saline (pH 8.5) was mixed with SCN-Bz-EDTA in a molar ratio of 1:5, and the mixture was incubated overnight at 30ºC. The excess agent was removed by applying the mixture to PD-10 gel chromatography. Conjugated antibody was then labeled with ^111^In. The radioactive ^111^In was prepared by incubating HCI, sodium acetate, and ^111^InCI_3_ for 1 h at room temperature. The ^111^In-labeled antibody was purified with chromatography on PD-10 gel. The isotype-matched control antibody FLOPC21 was also radiolabeled under the same conditions (^111^In-FLOPC21). FLOPC21 is a purified mouse myeloma protein IgG3κ. The specific activity and labeling efficiency values of the radioactive antibodies were ~74 MBq/mg (2 mCi/mg) and >99%, respectively. The purity and stability of the radioactive antibodies were not reported.

## In Vitro Studie: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Yao et al. analyzed the ability of ^111^In-MLS128 to bind to the LS180 tumor cells in vitro by incubating them together for 1 h at 4ºC (4). The fraction of the immunoreactive antibody was determined with linear extrapolation to conditions representing infinite antigen excess. The immunoreactive fraction is a parameter used for quality control of antibody radiolabeling (22); it represents how much of the conjugated antibody is able to bind to the relevant antigen. In vitro studies have shown that the immunoreactive fraction of ^111^In-MLS128 was 53.1%. The affinity constant of ^111^In-MLS128 was not reported. No blocking study was reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Biodistribution of ^111^In-MLS128 and the control ^111^In-FLOPC21 was studied in female BALB/c nu/nu mice bearing LS180 subcutaneous tumor xenografts (4). Potassium iodide solution was administered to mice 1 day before injection of the antibodies. ^111^In-MLS128 (10 µg, 37 kBq (1 µCi)) was administered via the tail vein. The mice were then euthanized at 24, 48, and 96 h after injection (n = 4 mice/time point), and the radioactivity in each organ was measured. The data showed that ^111^In-MLS128 was well localized the tumors. Accumulation of ^111^In-MLS128 in tumors was rapid and high at 24.16 ± 6.24% injected dose per gram of tissue (ID/g) at 24 h, reaching a peak of 31.05 ± 3.02% ID/g at 48 h after injection. The ratios of tumor/nontumor radioactivity at 48 h reached 3.92, 2.90, and 20.98 for blood, liver, and bone, respectively, and increased thereafter. The biodistribution of the control ^111^In-FLOPC21 in normal organs was similar to that of ^111^In-MLS128, but the tumor uptake of ^111^In-FLOPC21 was very low at only 6.43 ± 0.32% ID/g at 48 h after injection. Yao et al. concluded that the anti-Tn MLS128 mAb is promising for radioimmunoimaging of colorectal cancer (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Springer G.F. (1997). Immunoreactive T and Tn epitopes in cancer diagnosis, prognosis, and immunotherapy. J Mol Med.
2 Ando H., Matsushita T., Wakitani M., Sato T., Kodama-Nishida S., Shibata K., Shitara K., Ohta S. (2008). Mouse-human chimeric anti-Tn IgG1 induced anti-tumor activity against Jurkat cells in vitro and in vivo. Biol Pharm Bull.
3 Li Q., Anver M.R., Butcher D.O., Gildersleeve J.C. (2009). Resolving conflicting data on expression of the Tn antigen and implications for clinical trials with cancer vaccines. Mol Cancer Ther.
4 Yao Z., Sakahara H., Zhang M., Kobayashi H., Nakada H., Yamashina I., Konishi J. (1995). Radioimmunoimaging of colon cancer xenografts with anti-Tn monoclonal antibody. Nucl Med Biol.
5 Babino A., Oppezzo P., Bianco S., Barrios E., Berois N., Navarrete H., Osinaga E. (2000). Tn antigen is a pre-cancerous biomarker in breast tissue and serum in n-nitrosomethylurea-induced rat mammary carcinogenesis. Int J Cancer.
6 Hakomori S. (2001). Tumor-associated carbohydrate antigens defining tumor malignancy: basis for development of anti-cancer vaccines. Adv Exp Med Biol.
7 Kulkarni K.A., Sinha S., Katiyar S., Surolia A., Vijayan M., Suguna K. (2005). Structural basis for the specificity of basic winged bean lectin for the Tn-antigen: a crystallographic, thermodynamic and modelling study. FEBS Lett.
8 Kurtenkov O., Klaamas K., Rittenhouse-Olson K., Vahter L., Sergejev B., Miljukhina L., Shljapnikova L. (2005). IgG immune response to tumor-associated carbohydrate antigens (TF, Tn, alphaGal) in patients with breast cancer: impact of neoadjuvant chemotherapy and relation to the survival. Exp Oncol.
9 Lescar J., Sanchez J.F., Audfray A., Coll J.L., Breton C., Mitchell E.P., Imberty A. (2007). Structural basis for recognition of breast and colon cancer epitopes Tn antigen and Forssman disaccharide by Helix pomatia lectin. Glycobiology.
10 Dausset J., Moullec J., Bernard J. (1959). Acquired hemolytic anemia with polyagglutinability of red blood cells due to a new factor present in normal human serum (Anti-Tn). Blood.
11 Springer G.F., Desai P.R., Spencer B.D., Tegtmeyer H., Carlstedt S.C., Scanlon E.F. (1995). T/Tn antigen vaccine is effective and safe in preventing recurrence of advanced breast carcinoma. Cancer Detect Prev.
12 Slovin S.F., Ragupathi G., Musselli C., Olkiewicz K., Verbel D., Kuduk S.D., Schwarz J.B., Sames D., Danishefsky S., Livingston P.O., Scher H.I. (2003). Fully synthetic carbohydrate-based vaccines in biochemically relapsed prostate cancer: clinical trial results with alpha-N-acetylgalactosamine-O-serine/threonine conjugate vaccine. J Clin Oncol.
13 Cipolla L., Rescigno M., Leone A., Peri F., La Ferla B., Nicotra F. (2002). Novel Tn antigen-containing neoglycopeptides: synthesis and evaluation as anti tumor vaccines. Bioorg Med Chem.
14 Takahashi H.K., Metoki R., Hakomori S. (1988). Immunoglobulin G3 monoclonal antibody directed to Tn antigen (tumor-associated alpha-N-acetylgalactosaminyl epitope) that does not cross-react with blood group A antigen. Cancer Res.
15 Yao Z., Zhang M., Sakahara H., Saga T., Kobayashi H., Nakamoto Y., Toyama S., Konishi J. (1998). Increased streptavidin uptake in tumors pretargeted with biotinylated antibody using a conjugate of streptavidin-fab fragment. Nucl Med Biol.
16 Zhang M., Yao Z., Saga T., Sakahara H., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1998). Improved intratumoral penetration of radiolabeled streptavidin in intraperitoneal tumors pretargeted with biotinylated antibody. J Nucl Med.
17 Zhang M., Yao Z., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Effect of administration route and dose of streptavidin or biotin on the tumor uptake of radioactivity in intraperitoneal tumor with multistep targeting. Nucl Med Biol.
18 Nakamoto Y., Saga T., Sakahara H., Yao Z., Zhang M., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Three-step tumor imaging with biotinylated monoclonal antibody, streptavidin and 111In-DTPA-biotin. Nucl Med Biol.
19 Numata Y., Nakada H., Fukui S., Kitagawa H., Ozaki K., Inoue M., Kawasaki T., Funakoshi I., Yamashina I. (1990). A monoclonal antibody directed to Tn antigen. Biochem Biophys Res Commun.
20 Oppezzo P., Osinaga E., Tello D., Bay S., Cantacuzene D., Irigoin F., Ferreira A., Roseto A., Cayota A., Alzari P., Pritsch O. (2000). Production and functional characterization of two mouse/human chimeric antibodies with specificity for the tumor-associated Tn-antigen. Hybridoma.
21 Zhang M., Sakahara H., Yao Z., Saga T., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1997). Intravenous avidin chase improved localization of radiolabeled streptavidin in intraperitoneal xenograft pretargeted with biotinylated antibody. Nucl Med Biol.
22 Lindmo T., Boven E., Cuttitta F., Fedorko J., Bunn P.A. (1984). Determination of the immunoreactive fraction of radiolabeled monoclonal antibodies by linear extrapolation to binding at infinite antigen excess. J Immunol Methods.